# Cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys-Cy5.5

Chemical name: | Cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys-Cy5.5
Abbreviated name: | Cy5.5-cNGR
Synonym:
Agent category: | Peptide
Target: | Aminopeptidase N (CD13)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Tumor angiogenesis represents a continuous and important process in tumor development in which the tumor attempts to gain an independent blood supply (4). This process is driven by the tumor's overproduction of angiogenic factors, which bind to receptors on nearby vessel endothelial cells. Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (5-7). Aminopeptidase N (APN, CD13) is a membrane bound glycoprotein with MMP activity that cleaves unsubstituted, N-terminal amino acids with neutral side chains from peptides (8). APN has been shown to play a role in tumor angiogenesis, invasion, and metastasis (9). In addition to endothelial cells of angiogenic vessels, most cells of myeloid origin, epithelial cells, fibroblasts and smooth muscle cells also express CD13 (10, 11). The tumor homing peptide cyclo(Cys-Asn-Gly-Arg-Cys)-Gly-Lys (cNGR) contains the Asn-Gly-Arg (NGR) motif that binds to APN (12). von Wallbrunn et al. (13) prepared Cy5.5-labeled cNGR (Cy5.5-cNGR) for imaging APN expression in tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+synthesis)]

Cy5.5 Monofunctional N-hydroxysuccinimide ester was used to conjugate cNGR to form Cy5.5-cNGR, which was purified with high-performance liquid chromatography with >95% purity (13). Cy5.5-cNGR was adjusted to a final concentration of 2 mg/ml. A molar ratio of Cy5.5 to cNGR was estimated to be ~1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+in+vitro)]

Histoimmunostaining of CD13 was performed on HT-1080 and MCF-7 cancer cell lines (13). The APN enzyme was expressed on the cell surface of HT-1080 tumor cells, whereas expression in MCF-7 tumor cells was only background staining. The APN activity in HT-1080 cells could be blocked with anti-CD13 antibodies and the cNGR peptide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+rodentia)]

von Wallbrunn et al. (13) performed ex vivo biodistribution studies of Cy5.5-cNGR in nude mice (n = 6) bearing HT-1080 fibrosarcoma tumors. Near-infrared fluorescence was measured in tumor, muscle, heart, lung, spleen, kidney, and liver at 24 h after injection of 2 nmol Cy5.5-cNGR. The organ with the highest concentration was the kidney (793 ± 272 AU), followed by the liver (398 ± 87 AU), tumor (332 ± 152 AU), and lung (307 ± 39 AU). Pretreatment with cNGR (10 mg/kg) 10 min before Cy5.5-cNGR injection resulted in decreased uptake in all dissected tissues. A similar distribution pattern was found in mice (n = 5) bearing MCF-7 tumors except lower fluorescence signal in the MCF-7 tumors (220 ± 10 AU) and kidney (500 ± 50 AU). Three-dimensional fluorescence-mediated tomography were also performed in mice bearing the tumor xenografts, showing an average Cy5.5-cNGR concentration of 307 ± 54 nM Cy5.5 (HT-1080) and 116 ± 18 nM Cy5.5 (MCF-7) in the tumors after 5 h. Pretreatment with cNGR (10 mg/kg) resulted in a reduction of tracer concentration in HT-1080 tumor tissue (195 ± 22 nM) at 5 h after injection. The tumor/background ratio was 7.5 ± 4.0 for Cy5.5-cNGR alone and 3.3 ± 2.1 for Cy5.5-cNGR with cNGR blocking. Histoimmunostaining of CD13 was performed on HT-1080 and MCF-7 tumor sections at 24 h after injection of Cy5.5-cNGR. The APN enzyme was expressed in HT-1080 tumor cells with intense membrane Cy5.5 fluorescence; whereas MCF-7 tumor cells exhibited marginal APN expression and Cy5.5 signal.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cNGR+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
5 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
6 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
7 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
8 Riemann D., Kehlen A., Langner J. (1999). CD13--not just a marker in leukemia typing. Immunol Today.
9 Sato Y. (2004). Role of aminopeptidase in angiogenesis. Biol Pharm Bull.
10 Corti A., Curnis F., Arap W., Pasqualini R. (2008). The neovasculature homing motif NGR: more than meets the eye. Blood.
11 Curnis F., Arrigoni G., Sacchi A., Fischetti L., Arap W., Pasqualini R., Corti A. (2002). Differential binding of drugs containing the NGR motif to CD13 isoforms in tumor vessels, epithelia, and myeloid cells. Cancer Res.
12 Arap W., Pasqualini R., Ruoslahti E. (1998). Cancer treatment by targeted drug delivery to tumor vasculature in a mouse model. Science.
13 von Wallbrunn A., Waldeck J., Holtke C., Zuhlsdorf M., Mesters R., Heindel W., Schafers M., Bremer C. (2008). In vivo optical imaging of CD13/APN-expression in tumor xenografts. J Biomed Opt.